# ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Phe(4-NO_2_)-cyclo(D-Cys-Tyr-D-Trp-Lys-Thr-Cys)-D-Tyr-NH_2_

Chemical name: | ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Phe(4-NO_2_)-cyclo(D-Cys-Tyr-D-Trp-Lys-Thr-Cys)-D-Tyr-NH_2_
Abbreviated name: | ^111^In-DOTA-sst_2_-ANT
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (sst_2_)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (sst_1_–sst_5_) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Labeled diethylenetriaminepentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SST analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). Octreotide (OCT) is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree, but it does not bind to sst_1_ and sst_4_ (8). Currently used targeting SSTR peptides mainly are sst_2_ agonists. Therefore, there is a need for sst_2_ antagonist radioligands (9). Ginj et al. (10) have developed a series of SST antagonist ligands. One of them, Phe(4-NO_2_)-cyclo(D-Cys-Tyr-D-Trp-Lys-Thr-Cys)-D-Tyr-NH_2_ (sst_2_-ANT), was found to be a selective sst_2_ antagonist. For evaluation as a SPECT imaging agent for sst_2_, ^64^Cu has been attached to sst_2_-ANT via tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^111^In-DOTA-sst_2_-ANT.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+synthesis)]

DOTA-sst_2_-ANT was synthesized via standard solid-phase peptide synthesis (10). DOTA was incorporated at the N-terminus of the peptide. DOTA-sst_2_-ANT was purified with high-performance liquid chromatography. Radiolabeling of DOTA-sst_2_-ANT with ^111^In was not reported. ^111^In-DOTA-sst_2_-ANT had a specific activity of ~20 GBq/µmol (0.54 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+in+vitro)]

Ginj et al. (10) reported that In-DOTA-sst_2_-ANT had 50% inhibition concentration (IC_50_) values of >1,000, 9.4 ± 0.4, >1,000, 380 ± 57, and >1,000 nM for human sst_1_, sst_2_, sst_3_, sst_4_, and sst_5_ receptors in competition with ^125^I-SRIF-28, respectively. Wadas et al. (11) determined that ^64^Cu-CB-TE2A-sst_2_-ANT showed a K_d_ (affinity constant) value of 26.0 ± 2.4 nM and a B_max_ (receptor density) value of 23 pmol/mg protein in AR42J (sst_2_-positive) tumor cell homogenates.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+rodentia)]

Ginj et al. (10) performed ex vivo biodistribution studies with ^111^In-DOTA-sst_2_-ANT in nude mice (n = 3/group) bearing xenografts of HEK-sst_2_ cells at 0.5, 4, and 24 h after injection. The accumulation of radioactivity in the sst_2_ tumors was 22.33% injected dose per gram (% ID/g) at 0.5 h, 29.12% ID/g at 4 h, and 22.84% ID/g at 24 h after injection. The pituitary was the organ that had the highest accumulation (20.33% ID/g) at 4 h after injection, followed by the kidney (10.50% ID/g), bone (1.29% ID/g), pancreas (0.71% ID/g) stomach (0.61% ID/g), and adrenal (0.49% ID/g). Accumulation of radioactivity in the other tissues was low. The concentration in the blood was 0.13% ID/g at 4 h after injection, with a tumor/blood ratio of 208 and a tumor/muscle ratio of 265 at 4 h after injection. Co-injection with DOTA-sst_2_-ANT reduced the accumulation of radioactivity by 88% in the tumors, 50% in the adrenal and bone, 66% in the stomach, 88% in the pancreas, and 85% in the pituitary at 4 h after injection. Little or no inhibition was observed in the other tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst2-ANT+and+human)]

No publication is currently available.

## NIH Support

R24 CA83060, F32 CA115148, R01 CA064475, R01 EB 1430, R24 CA86307

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.
11 Wadas T.J., Eiblmaier M., Zheleznyak A., Sherman C.D., Ferdani R., Liang K., Achilefu S., Anderson C.J. (2008). Preparation and biological evaluation of 64Cu-CB-TE2A-sst2-ANT, a somatostatin antagonist for PET imaging of somatostatin receptor-positive tumors. J Nucl Med.